# 7-(2-(4-(2-Fluoro-4-[^123^I]iodophenyl)piperazin-1-yl)ethyl)-2-(furan-2-yl)-7H-pyrazolo[4,3-e][1,2,4]triazolo[1,5-c]pyrimidin-5-amine

Chemical name: | 7-(2-(4-(2-Fluoro-4-[^123^I]iodophenyl)piperazin-1-yl)ethyl)-2-(furan-2-yl)-7H-pyrazolo[4,3-e][1,2,4]triazolo[1,5-c]pyrimidin-5-amine
Abbreviated name: | [^123^I]MNI-420
Synonym:
Agent Category: | Compound
Target: | Adenosine 2A (A_2A_) receptor
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^123^I
Activation: | No
Studies: | - In vitro; - Non-human primates | Click on the structure of [^123^I]MNI-420 for more information in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=a2a%20adenosine%20receptors&cmd=DetailsSearch)]

Free adenosine is a purinergic neurotransmitter that acts in conjunction with and modulates the activity of other central nervous system neurotransmitters, such as dopamine, glutamate, and acetylcholine, in areas that control motor function, mood, and learning and memory (1). Adenosine mediates its activity through four sub-types of G-protein–coupled receptors designated A_1_, A_2A_, A_2B_, and A_3_. The A_1_ and A_3_ sub-types are stimulatory receptors, whereas the A_2A_ and A_2B_ are the inhibitory sub-type of G-protein–coupled receptors (1). The biological and pharmacological characteristics of only the A_1_ and A_2A_ receptors in rodent and human brains have been well studied (2). Although A_1_ receptors are present in most sections of the brain, positron emission tomography (PET) imaging has shown that A_2A_ receptors are found primarily in the striatum, nucleus accumbens, and the olfactory tubercle regions of this organ (2, 3). In the striatum, the A_2A_ receptors are closely associated with the dopamine D_2_ receptors, and the A_2A_ receptors have an opposite effect on D_2_ receptor–mediated neurotransmissions; agonists of A_2A_ receptors are known to block the neurotransmission activity of D_2_ receptors, and inhibitors of the A_2A_ receptors are known to upregulate D_2_ receptor activity (1). There are indications that abnormal A_2A_ receptor activity is responsible for the development of neurodegenerative conditions in humans, such as Parkinson’s disease and Huntington’s disease. Several clinical trials are in progress to evaluate the efficacy of A_2A_ receptor antagonists for the treatment of Parkinson’s disease (4).

Several radiotracers have been developed and evaluated with PET for the noninvasive imaging of A_2A_ receptors in rodents and monkeys, but none of these probes have been deemed suitable for the imaging of these receptors in the non-human primates (2). Only two ^11^C-labeled compounds, 5-amino-7-(3-(4-[^11^C]methoxy)phenylpropyl)-2-(2-furyl)pyrazolo[4,3-e]-1,2,4-triazolo[1,5-c]pyrimidine (5) and 7-methyl-[^11^C]-(E)-8-(3,4,5-trimethoxystyryl)-1,3,7-trime​thylxanthine (6), are considered acceptable for the imaging of A_2A_ receptors in humans with Parkinson’s disease (2). However, these radiochemicals cannot be used in most clinics because most clinics do not have the cyclotron facilities that are required for preparation of the ^11^C-labeled compounds. In this regard, radionuclides such as ^123^I-labeled agents are easily available from a central pharmacy, do not have to be generated on-site, and can be used for noninvasive imaging with single-photon emission computed tomography (SPECT) (2). Therefore, it was proposed that SPECT probes would be more useful for the imaging of A_2A_ receptors in the clinic (2). On the basis of this proposal, a novel, ^123^I-labeled SPECT tracer, 7-(2-(4-(2-fluoro-4-[^123^I]iodophenyl)piperazin-1-yl)ethyl)-2-(furan-2-yl)-7H-pyrazolo[4,3-e][1,2,4]triazolo[1,5-c]pyrimidin-5-amine ([^123^I]MNI-420) was synthesized and evaluated for the imaging of A2A receptors in two species of non-human primates (2).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=A2A+receptor+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Protein (http://www.ncbi.nlm.nih.gov/protein/NP_000666.2) and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/NM_000677.3) sequences of human adenosine A_2A_ receptor

Human adenosine A_2A_ receptor in Gene Database (http://www.ncbi.nlm.nih.gov/gene/135), Gene ID: 135

Adenosine A_2A_ receptor in Online Mendelian Inheritance in Man Database (OMIM (http://omim.org/entry/102776))

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Adenosine+a2a+receptors&Search=Search) related to adenosine A_2A_ receptors

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=123I-MNI-420%20synthesis&cmd=DetailsSearch)]

The synthesis of [^123^I]MNI-420 has been described by Tavares et al. (2). The final radiolabeled product was purified with high-performance liquid chromatography and formulated in 0.9% sodium chloride. The radiochemical yield, radiochemical purity, and specific activity of [^123^I]MNI-420 at the end of synthesis were reported to be ~49%, >95%, and 7.4 TBq/μmol (2.0 Ci/μmol), respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=123I-MNI-420+in+vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=123I-MNI-420%20rodentia&cmd=DetailsSearch)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=23332393%5Buid%5D&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=23332393%5Buid%5D&cmd=DetailsSearch)]

Increasing doses of caffeine (2–20 mg/kg body weight (BW)) were used to determine SPECT baseline and [^123^I]MNI-420 displacement characteristics in the brains of three ovariectomized adult female baboons (Papio anubis) (2). For the baseline study, the anesthetized baboons were given bolus intravenous (i.v.) injections of ~461 ± 128 MBq (12.45 ± 3.45 mCi) [^123^I]MNI-420, and SPECT images of the animals were acquired for up to 3 h postinjection (p.i.). SPECT images from the baseline study showed that the radioactivity from [^123^I]MNI-420 entered the brain rapidly and peaked at ~30 min p.i. A baseline was considered to have been established when the target/non-target ratios reached pseudoequilibrium at ~90 min p.i. The uptake of tracer corresponded to the distribution of A_2A_ receptor in the various regions of the brain; it was highest in the striatum, low in the cortical sections, and negligible in the cerebellum. The mean standardized uptake value ratio (SUVr) of the striatal and cortical tissues with respect to the cerebellum at pseudoequilibrium were determined to be 2.96 ± 0.62. For the displacement study, the animals were given a single bolus i.v. injection of different doses of caffeine (a competitive inhibitor of adenosine) at ~90 min after treatment with [^123^I]MNI-420, and SPECT images of the animals were acquired for up to 90 min after the caffeine injection. The amount of label in the target region of the brain was reduced by caffeine in a dose-dependent manner, and at a dose of 20 mg/kg BW the caffeine was reported to occupy ~98% of A_2A_ receptors. The 50% effective dose (ED_50_) of caffeine for the A_2A_ receptors in the baboons was determined to be ~3.8 mg/kg BW.

Blocking studies with preladenant (an antagonist of A_2A_ receptor) were performed on two adult male cynomolgus monkeys (Macaca fascicularis) as described elsewhere (2). The monkeys were given a bolus i.v. injection of 131 ± 55 MBq (3.54 ± 1.48 mi) [^123^I]MNI-420, and SPECT images were obtained from the animals for up to 4 h p.i. The rate and pattern of uptake of label in the brain of these monkeys were similar to those observed with the baboons. The striatum/cerebellum SUVrs for monkey 1 and monkey 2 at 90 min p.i. were 3.5 and 3.0, respectively. For the blocking study, monkey 1 was injected only with preladenant (0.01–1.0 mg/kg BW), and monkey 2 was injected with preladenant (0.01–1.2 mg/kg BW) 15 min prior to the treatment with [^123^I]MNI-420. SPECT images of both monkeys were acquired at baseline and once each after pretreatment with preladenant. Pretreatment with preladenant reduced the amount of label accumulated in the striatum of both animals in a dose-dependent manner. Approximately 97% of A_2A_ receptors were occupied by preladenant at a dose of 1.2 mg/kg BW. The ED_50_ of preladenant was calculated to be 0.05 mg/kg BW. This indicated that [^123^I]MNI-420 had a high binding selectivity for A_2A_ receptors.

From these studies, the investigators concluded that [^123^I]MNI-420 is probably suitable for the characterization of A_2A_ receptors in the non-human primate brain, though further evaluation of the tracer is necessary to establish its utility as a SPECT imaging agent of the receptor (2).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=23332393%5Buid%5D&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Shook B.C., Jackson P.F. (2011). Adenosine A(2A) Receptor Antagonists and Parkinson's Disease. ACS Chem Neurosci.
2 Tavares A.A., Batis J., Barret O., Alagille D., Vala C., Kudej G., Koren A., Cosgrove K.P., Nice K., Kordower J.H., Seibyl J., Tamagnan G.D. (2013). In vivo evaluation of [(123)I]MNI-420: A novel single photon emission computed tomography radiotracer for imaging of adenosine 2A receptors in brain. Nucl Med Biol.
3 Moresco R.M., Todde S., Belloli S., Simonelli P., Panzacchi A., Rigamonti M., Galli-Kienle M., Fazio F. (2005). In vivo imaging of adenosine A2A receptors in rat and primate brain using [11C]SCH442416. Eur J Nucl Med Mol Imaging.
4 Chen J.F., Eltzschig H.K., Fredholm B.B. (2013). Adenosine receptors as drug targets - what are the challenges?. Nat Rev Drug Discov.
5 Ramlackhansingh A.F., Bose S.K., Ahmed I., Turkheimer F.E., Pavese N., Brooks D.J. (2011). Adenosine 2A receptor availability in dyskinetic and nondyskinetic patients with Parkinson disease. Neurology.
6 Mishina M., Ishiwata K., Naganawa M., Kimura Y., Kitamura S., Suzuki M., Hashimoto M., Ishibashi K., Oda K., Sakata M., Hamamoto M., Kobayashi S., Katayama Y., Ishii K. (2011). Adenosine A(2A) receptors measured with [C]TMSX PET in the striata of Parkinson's disease patients. PLoS One.